# ^177^Lu-DOTA-Gly-4-aminobenzoyl-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_

Chemical name: | ^177^Lu-DOTA-Gly-4-aminobenzoyl-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_
Abbreviated name: | [^177^Lu]-AMBA
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRP-R)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal/contrast: | ^177^Lu
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=177Lu-AMBA)]

Bombesin (BBN) is a tetradecapeptide isolated from the European fire-bellied frog (Bombina bombina) (1). BBN possesses a specific C-terminus (Gly-His-Leu-Met), which is necessary for its biological activity (2). Several peptides that are structurally related to BBN have been identified in mammals. Gastrin-releasing peptide (GRP) is a peptide of 27 amino acids from porcine gastric tissues with Gly-His-Leu-Met at its C-terminus. Neuromedin B (NMB) is a peptide of 32 amino acids from porcine spinal cords with Gly-His-Phe-Met at its C-terminus. These peptides are the ligands of a group of receptors called BBN receptors (BB-R). The mammalian BB-R family consists of three subtypes, including the GRP-preferring receptor (GRP-R or BB_2_-R (384 amino acids)), the NMB-preferring receptor (NMB-R or BB_1_-R (390 amino acids)), and an orphan receptor (BB_3_-R (399 amino acids)) (3). These subtypes of BB-R are overexpressed in various diseased tissues. For example, GRP acts as a neurotransmitter and an endocrine cell-growth factor to regulate various functions of gastrointestinal and central nervous systems and to stimulate cell proliferations in lung, colon, stomach, pancreas, breast, and prostate cancers in humans (4). GRP binds to GRP-R as an agonist and is subsequently transported to the perinuclear space via receptor-mediated endocytosis (1), which leads to an accumulation in GRP-R–positive tissues. Thus, tagging GRP with an imaging probe allows for assessment of GRP-R in vivo.

^177^Lu-(4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetracetic acid (DOTA))-Gly-4-aminobenzoyl-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_ (^177^Lu-AMBA) is used with single-photon emission computed tomography (SPECT) imaging of GRP-R (5). ^177^Lu-AMBA consists of two components: a peptide of eight amino acids that is composed of the seven common amino acids in the C-terminus of BBN/GRP (Trp-Ala-Val-Gly-His-Leu-Met) and a complex of ^177^Lu-DOTA attached to the N-terminus of the peptide via a glycyl-4-aminobezoic acid linker. The small peptide accounts for the biological potency and possesses many advantages such as high in vivo stability, high uptake in tumors, low uptake in non-target tissues, and a rapid clearance from blood via the kidney (3). ^177^Lu is a radionuclide from the group of rare earth radionuclides, and it is produced by neutron bombardment of purified target material in reactors (6). With a half-life of 6.71 days for β^-^ emission at 498 keV and 78% branch fraction, ^177^Lu has been a very promising radionuclide in radiotherapy for effective destruction of small tumors and metastasis (optimal size 1.2–3.0 mm) while sparing normal tissue (7). ^177^Lu also emits low-energy gamma rays at 208 and 113 keV with 10% and 6% abundance, respectively, which allows for direct monitoring of the activity distribution with SPECT and subsequent dosimetry calculations. ^177^Lu-AMBA is currently under phase I clinical trials (8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177Lu-AMBA)+AND+synthesis%0D%0A)]

Lantry et al. reported the synthesis of ^177^Lu-AMBA (5). AMBA was produced with solid-phase peptide synthesis at a 14.5% yield followed by reaction with ~2.2 GBq (59.4 mCi ) ^177^LuCl_3_ with specific activity of 103.6-151.3 GBq/μmol (2.8–4.09 Ci/μmol) in 0.05 N HCl for 10 min at 100ºC. The produced ^177^Lu-AMBA was purified with high-performance liquid chromatography (HPLC).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177Lu-AMBA)+AND+%22in+vitro%22)]

Lantry et al. examined the specificity of in vitro ^177^Lu-AMBA binding to GRP-R in human prostate cancer PC-3 cells (~2.5 × 10^5^ GRP-R per cell) (5). The 50% inhibition concentration (IC_50_) was measured via competition studies in which six cold metalated ligand (^175^Lu-AMBA) solutions ranging from 1.25 × 10^-9^ M to 5.0 × 10^-8^ M were used to inhibit the binding of ^125^I-[Tyr^4^]-BBN with specific activity of 2.2 Ci/μmol (81.4 GBq/μmol). The binding affinity (K_d_) and the maximum binding capacity (B_max_) were measured via direct saturation studies, in which 10 ^177^Lu-AMBA solutions ranging from 0.0-0.37 MBq/ml (0–0.01 Ci/ml) were used. Both the inhibitory and the saturation studies were performed at 4ºC to eliminate interference from internalization and degradation. The measured IC_50_, K_d_, and B_max_ values were 2.50 ± 0.50 nmol/L, 1.02 nmol/L, and 414 fmol per 10^6^ PC-3 cells, respectively. The internalization of ^177^Lu-AMBA was evaluated in adherent PC-3 cells at 37ºC. After 40 min of incubation, 76.8 ± 1.8% of ^177^Lu-AMBA was internalized. Only 2.9 ± 1.8% was effluxed in 2 h; most (78%) remained in the form of parent ^177^Lu-AMBA as found with HPLC. ^177^Lu-AMBA appeared to be very stable; its half-life time was 38.8 h in human plasma and 3.1 h in mouse plasma. The specificity of ^177^Lu-AMBA binding to BB-R subtypes was examined with receptor autoradiography in vitro. Tissue sections of human ileal carcinoid (NMB-R), human prostate carcinoma (GRP-R), and human bronchial carcinoid (BB_3_-R) were used for studies. ^177^Lu-AMBA bound specifically to GRP-R (IC_50_, 0.8 nmol) and NMB-R (IC_50_, 0.9 nmol/L) at high affinities, but less exhibited less preference for BB_3_-R (IC_50_ >1,000 nmol).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177Lu-AMBA) +AND++rodentia)]

Lantry et al. evaluated the biodistribution of ^177^Lu-AMBA in mice in vivo (5). Nude mice (age 4–6 wk, n = 4) bearing PC-3 tumors (~0.5 g) were intravenously injected with ^177^Lu-AMBA 0.185 MBq/ml with specific activity of 118.4 GBq/μmol (3.2 Ci/μmol). At 1 h or 24 h after injection, mice were euthanized and the tissues were harvested for gamma counting of residual radioactivity. At 1 h, measured radioactivity (percentage of injected dose (% ID)) was found to be 6.35 ± 2.23 in tumor, 0.46 ± 0.20 in blood, 0.25 ± 0.08 in liver, 2.95 ± 0.79 in kidney, 17.78 ± 4.07 in pancreas, 11.22 ± 3.29 in gastrointestine, and 55.66 ± 7.28 in bladder/urine. At 24 h, measured radioactivity was 3.39 ± 0.85 in tumor, 0.03 ± 0.02 in blood, 0.21 ± 0.368 in liver, 0.91 ± 0.25 in kidney, 12.28 ± 3.5 in pancreas, and 5.77 ± 1.79 in gastrointestine; no detectable amount was found in bladder/urine. ^177^Lu-AMBA was excreted primarily via the kidney.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177Lu-AMBA) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177Lu-AMBA) +AND+human)]

No publication is currently available.

## References

1 Varvarigou A., Bouziotis P., Zikos C., Scopinaro F., De Vincentis G. (2004). Gastrin-releasing peptide (GRP) analogues for cancer imaging. Cancer Biother Radiopharm.
2 Ohki-Hamazaki H., Iwabuchi M., Maekawa F. (2005). Development and function of bombesin-like peptides and their receptors. Int J Dev Biol.
3 Dijkgraaf I., Boerman O.C., Oyen W.J., Corstens F.H., Gotthardt M. (2007). Development and application of peptide-based radiopharmaceuticals. Anticancer Agents Med Chem.
4 Smith C.J., Gali H., Sieckman G.L., Hayes D.L., Owen N.K., Mazuru D.G., Volkert W.A., Hoffman T.J. (2003). Radiochemical investigations of 177Lu-DOTA-8-Aoc-BBN[7-14]NH2: an in vitro/in vivo assessment of the targeting ability of this new radiopharmaceutical for PC-3 human prostate cancer cells. Nucl Med Biol.
5 Lantry L.E., Cappelletti E., Maddalena M.E., Fox J.S., Feng W., Chen J., Thomas R., Eaton S.M., Bogdan N.J., Arunachalam T., Reubi J.C., Raju N., Metcalfe E.C., Lattuada L., Linder K.E., Swenson R.E., Tweedle M.F., Nunn A.D. (2006). 177Lu-AMBA: Synthesis and characterization of a selective 177Lu-labeled GRP-R agonist for systemic radiotherapy of prostate cancer. J Nucl Med.
6 Schotzig U., Schrader H., Schonfeld E., Gunther E., Klein R. (2001). Standardisation and decay data of 177Lu and 188Re. Appl Radiat Isot.
7 Dvorakova Z., Henkelmann R., Lin X., Turler A., Gerstenberg H. (2008). Production of 177Lu at the new research reactor FRM-II: Irradiation yield of 176Lu(n,gamma)177Lu. Appl Radiat Isot.
8 Waser B., Eltschinger V., Linder K., Nunn A., Reubi J.C. (2007). Selective in vitro targeting of GRP and NMB receptors in human tumours with the new bombesin tracer 177Lu-AMBA. Eur J Nucl Med Mol Imaging.